# ^99m^Tc-Tricarbonyl–labeled aspartic-N-monoacetic acid (ASMA)

Chemical name: | ^99m^Tc-Tricarbonyl–labeled aspartic-N-monoacetic acid (ASMA) | [image]
Abbreviated name: | [^99m^Tc](CO)_3_(ASMA) | [image]
Synonym: | | [image]
Agent Category: | Compound | [image]
Target: | Organic anion transporter 1 (OAT1) | [image]
Target Category: | Transporter | [image]
Method of detection: | Single-photon emission computed tomography (SPECT); gamma planar imaging | [image]
Source of signal / contrast: | ^99m^Tc | [image]
Activation: | No | [image]
Studies: | - In vitro; - Rodents | Structure of ASMA (1)

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=%5B99mTc%5D%28CO%293%28ASMA%29&cmd=DetailsSearch)]

Ortho-[^131^I]-iodohippurate ([^131^I]-OIH) is considered to be the gold standard for the noninvasive imaging of kidney function and the detection of nephro-urological diseases in humans (2). However, because [^131^I]-OIH can deliver a high dose of radiation to the kidneys and the thyroid, especially in patients with an impaired renal function, this radiolabeled compound is no longer available for clinical use in many countries (1). In the United States, ^99m^ Tc-labeled mercaptoacetylglycylglycylglycine ([^99m^Tc]-MAG_3_) is often used with gamma planar imaging to assess renal function in individuals, but this tracer generates a low signal/background ratio from the kidneys due to a differential attenuation of the ^99m^Tc-gamma radiation between the two organs (3). In addition, data generated from these scans do not allow accurate quantification of kidney function because the renal clearance of [^99m^Tc]-MAG_3_ is only 50%–60% that of [^131^I]-OIH (1).

A ^99m^Tc-tricarbonyl–labeled nitrilotriacetic acid (NTA)–based renal imaging agent ([^99m^Tc](CO)_3_(NTA)) was shown to be equivalent to [^131^I]-OIH for the assessment of kidney function in normal rats (4) and human volunteers (5). However, the use of [^99m^Tc](CO)_3_(NTA) in patients with a clinically diminished renal capacity has not been evaluated. In an effort to develop a radiolabeled imaging agent that can be used to assess impaired renal function, an isomer of [^99m^Tc](CO)_3_(NTA), [^99m^Tc](CO)_3_(aspartic-N-monoacetic acid) ([^99m^Tc](CO)_3_(ASMA)), was developed, and the biodistribution of [^99m^Tc](CO)_3_(ASMA) was investigated in normal rats and a rats that model of renal failure (1).

### Related Resource Links

Related chapters in MICAD (http://www.ncbi.nlm.nih.gov/books/?term=fluorohippurate+AND+micad%5Bbook%5D&view=chapter&p%24a=&p%24l=PBooksLayout&p%24st=books)

References for [^131^I]-iodohippurate in PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=131I-iodohippurate&cmd=DetailsSearch)

References for [^99m^Tc]-MAG_3_ in PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=99mTc-MAG3&cmd=DetailsSearch)

Clinical trials (http://clinicaltrials.gov/ct2/results?term=99mTc-MAG3+) with [^99m^Tc]-MAG_3_

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=%5B99mTc%5D%28CO%293%28ASMA%29%20synthesis&cmd=DetailsSearch)]

A racemic mixture of the D- and L-isomers of ASMA (rac-ASMA) and the enantiomerically pure L-ASMA were synthesized as described elsewhere (1). The ^99m^Tc-tricarbonyl complexes of rac-ASMA ([^99m^Tc](CO)_3_(rac-ASMA)) and L-ASMA ([^99m^Tc](CO)_3_(L-ASMA)) were prepared as detailed by Lipowska et al. (1). The radiochemical purity (RCP) of the two radiolabeled compounds was >99% as determined with high-performance liquid chromatography (HPLC). The radiochemical yields (RCY) and specific activities of [^99m^Tc](CO)_3_(rac-ASMA) and [^99m^Tc](CO)_3_(L-ASMA) were not reported.

The source, RCY, RCP, and specific activity of [^131^I]-OIH, which was used in the biodistribution studies for comparison purposes, were not reported (1).

In this chapter, the term [^99m^Tc](CO)_3_(ASMA) has been used as a general reference to the [^99m^Tc](CO)_3_(rac-ASMA) and [^99m^Tc](CO)_3_(L-ASMA) complexes.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=%5B99mTc%5D%28CO%293%28ASMA%29%20in%20vitro&cmd=DetailsSearch)]

The stability of the [^99m^Tc](CO)_3_(ASMA) tracers was evaluated by incubating the radiochemicals with or without cysteine or histidine in phosphate buffer (pH 7.4) for up to 24 h (1). HPLC analysis of aliquots obtained at various time points from the mixtures showed there was no decomposition of the radiochemical complexes for at least 4 h.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=%5B99mTc%5D%28CO%293%28ASMA%29%20rodentia&cmd=DetailsSearch)]

The biodistribution of [^99m^Tc](CO)_3_(ASMA) was investigated in normal rats (Group A) and a group of rats that modeled renal failure (Group B; the renal pedicles in these animals were ligated so that no urine was produced) (1). The rats (n = 4 anesthetized animals/group) were injected with a mixture of 0.74 MBq (20 μCi) [^99m^Tc](CO)_3_(ASMA) and 185 kBq (5 MCi) [^131^I]-OIH through the tail vein. Group A rats were euthanized at 10 min postinjection (p.i.) and at 60 min p.i., and the Group B animals were euthanized at 60 min p.i. to determine the amount of radioactivity accumulated in the tissues and organs of interest. Urine was also collected from these animals for the duration of the study as described by Lipowska et al. (1). The amount of radioactivity present in the various tissues and urine of the animals was presented as a percent of injected dose (% ID) as shown in Table 1. With both [^99m^Tc](CO)_3_(ASMA) preparations, the amount of radioactivity in the blood of Group A rats was comparable to that with [^131^I]-OIH (P = 0.07) at 10 min p.i.; however, at 60 min p.i. the amount of ^99m^Tc in the blood with both ^99m^Tc tracers was significantly lower (P < 0.003) than radioiodide. At 10 min p.i., the amount of radioactivity from the ^99m^Tc tracers in the urine was comparable to that from [^131^I]-OIH (P > 0.1). At 60 min p.i., the elimination of ^99m^Tc through the urine was significantly faster (P < 0.001) than that of ^131^I. The urinary ^99m^Tc/^131^I ratios at 10 min p.i. and 60 min p.i. were 106 ± 6 and 100 ± 3, and 106 ± 0 and 107 ± 2 for [^99m^Tc](CO)_3_(rac-ASMA) and [^99m^Tc](CO)_3_(L-ASMA), respectively. With the ^99m^Tc-labeled compounds, very low levels of radioactivity were detected in the other organs (only data for liver is presented in Table 1).

Table 1: Biodistribution of tracer from [ ^ 99m ^ Tc](CO) _ 3 _ (ASMA) presented as % ID in select tissues of normal rats (Group A) and rats with renal failure (Group B) ( 1 ).

Tissue, organ, or fluid | Group A | | | | Group B
Tissue, organ, or fluid | ^ 99m ^ Tc-rac-ASMA | ^ 99m ^ Tc-L-ASMA | ^ 99m ^ Tc-rac-ASMA | ^ 99m ^ Tc-L-ASMA | ^ 99m ^ Tc-rac-ASMA
Tissue, organ, or fluid | Time p.i.
Tissue, organ, or fluid | 10 min | | 60 min
Blood | 5.2 ± 1.7 (6.7 ± 1.9) | 4.7 ± 0.9 (5.1 ± 1.0) | 0.2 ± 0.0 (0.7 ± 0.1) | 0.3 ± 0.1 (0.8 ± 0.1) | 17.9 ± 1.1 (16.7 ± 1.3)
Liver | 2.5 ± 0.3 (3.7 ± 0.6) | 3.7 ± 1.2 (2.9 ± 0.3) | 0.2 ± 0.1 (0.7 ± 0.1) | 0.3 ± 0.0 (0.6 ± 0.2) | 6.2 ± 0.6 (7.9 ± 0.5)
Kidney | 6.7 ± 1.0 (6.5 ± 0.7) | 4.3 ± 2.2 (4.0 ± 1.8) | 0.2 ± 0.1 (0.3 ± 0.1) | 0.7 ± 0.3 (0.7 ± 0.3) | 0.6 ± 0.2 (0.5 ± 0.2)
Urine | 51.3 ± 6.2 (48.3 ± 4.9) | 51.1 ± 7.3 (50.9 ± 6.0) | 94.4 ± 1.0 (89.1 ± 0.9) | 95.1 ± 4.1 (88.8 ± 2.7) | –
% Urinary ^ 99m ^ Tc/ ^ 131 ^ I ratio | 106 ± 6 | 100 ± 3 | 106 ± 0 | 107 ± 2 | –

Values in parentheses represent % ID of radioactivity from [ ^ 131 ^ I]-OIH. ID: injected dose; p.i., postinjection.

Because the biodistribution of [^99m^Tc](CO)_3_(rac-ASMA) and [^99m^Tc](CO)_3_(L-ASMA) was similar in the normal rats, only [^99m^Tc](CO)_3_(rac-ASMA) was used for the biodistribution study in rodents with renal failure (Group B) (1). The Group B animals showed an increased accumulation of radioactivity in the liver and intestine both with [^99m^Tc](CO)_3_(rac-ASMA) and [^131^I]-OIH at 60 min p.i. Accumulation of the tracer was significantly higher with [^131^I]-OIH compared with [^99m^Tc](CO)_3_(rac-ASMA) (P = 0.032 and P = 0.019 for liver and intestine, respectively). This indicated that, compared with the ^99m^Tc-labeled tracer, the excretion of radioactivity from the ^131^I-labeled compound was primarily through the hepatobiliary route under renal failure conditions. In addition, the retention of label in the blood was significantly higher (P = 0.017) with [^99m^Tc](CO)_3_(rac-ASMA) than with [^131^I]-OIH.

From these studies, the investigators concluded that the biodistribution of the [^99m^Tc](CO)_3_(ASMA) complexes was quite similar to that of [^131^I]-OIH in normal rodents (1).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=%5B99mTc%5D%28CO%293%28ASMA%29%20Non-Primate%20Mammals&cmd=DetailsSearch)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=%5B99mTc%5D%28CO%293%28ASMA%29%20Non-Human%20Primates&cmd=DetailsSearch)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=%5B99mTc%5D%28CO%293%28ASMA%29%20Human%20Studies&cmd=DetailsSearch)]

No publication is currently available.

## Supplemental Information

[Disclaimers]

No information is currently available.

## NIH Support

Supported by grant R37 DK38842 from the National Institutes of Health.

## References

1 Lipowska, M., J. Klenc, L.G. Marzilli, and A.T. Taylor, Preclinical Evaluation of 99mTc(CO)3-Aspartic-N-Monoacetic Acid, a Renal Radiotracer with Pharmacokinetic Properties Comparable to 131I-o-Iodohippurate. J Nucl Med, 2012
2 Itoh K. (2001). 99mTc-MAG3: review of pharmacokinetics, clinical application to renal diseases and quantification of renal function. Ann Nucl Med.
3 Awasthi V., Pathuri G., Agashe H.B., Gali H. (2011). Synthesis and in vivo evaluation of p-18F-Fluorohippurate as a new radiopharmaceutical for assessment of renal function by PET. J Nucl Med.
4 Lipowska M., Marzilli L.G., Taylor A.T. (2009). 99mTc(CO)3-nitrilotriacetic acid: a new renal radiopharmaceutical showing pharmacokinetic properties in rats comparable to those of 131I-OIH. J Nucl Med.
5 Taylor A.T., Lipowska M., Marzilli L.G. (2010). (99m)Tc(CO)3(NTA): a (99m)Tc renal tracer with pharmacokinetic properties comparable to those of (131)I-OIH in healthy volunteers. J Nucl Med.